# Avidin-gadolinium

Chemical name: | Avidin-gadolinium
Abbreviated name: | Avidin-Gd
Synonym:
Agent Category: | Protein
Target: | Biotinylated anti-HER-2/neu antibody
Target Category: | Protein–protein binding
Method of detection: | Magnetic resonance imaging (MRI)
Source of Signal/Contrast: | Gadolinium
Activation: | No
Studies: | - In vitro; - Rodents | No information is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=avidin+Gd)]

Biotin is a protein found in mammalian cells and is considered to be a vitamin because it has an important function in the cellular metabolism of lipids and carbohydrates. Avidin is a protein that is found primarily in the egg white or in bacteria (known as streptavidin if isolated from bacteria; Streptomyces avidinii is the source of this protein). Although the two proteins have different origins, they are known to have a very strong non-covalent interaction (discovered almost seven decades ago) with a dissociation constant (K_d_) of 4 × 10^-14^ M (1, 2). The avidin–biotin interaction has been described in detail by Wilchek et al. (3). Only harsh conditions (e.g., treatment with formaldehyde at high temperature) are known to break the avidin/streptavidin–biotin bond, and the released proteins cannot be reused for any other work due to deterioration of the samples (4). Because of their strong interaction, the avidin/streptavidin–biotin system has been extensively studied and is widely used after conjugation of either protein to other proteins, nucleic acids, or other matrices for research and diagnostic purposes, including imaging techniques (5-8).

Because of its overexpression, the human epidermal growth factor receptor 2 (HER2/neu) is an important target for the diagnosis, treatment, and prognosis of cancers such as those of the breast, lungs, etc (9, 10). As a result, humanized monoclonal antibodies (MAbs) labeled with different nuclides or imaging and contrast agents targeted toward HER2/neu have been used for the in vitro and in vivo imaging of cancers (11-13). Some humanized MAbs against HER2/neu alone or their conjugated derivatives are used, or are in development, as immunotherapeutic agents for the treatment of this ailment (14, 15). The avidin–biotin system has been used to visualize HER2/neu-positive tumors in transgenic mice by some investigators with magnetic resonance imaging (MRI) (16, 17). To achieve this, the investigators prelabeled the cells expressing HER2/neu, under in vitro and in vivo conditions, with a commercially available biotinylated mouse MAb. The biotinylated MAb was allowed to wash or clear out from the respective test systems, and this was followed by the administration of avidin conjugated to gadolinium (avidin-Gd) to the cells or animals. MRI was subsequently performed, and it was demonstrated that a high positive T1 contrast could be achieved under the in vitro and in vivo conditions used.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=avidin+gadolinium+synthesis)]

The synthesis of avidin-Gd was performed as described by Artemov et al. using a modified procedure of Hnatowich et al. (13, 18). Briefly, 20-fold excess cyclic anhydride of diethylenetriaminepentaacetic acid (DTPA) was allowed to react with avidin for 24 h at 4°C. Excess low molecular weight reagents from the conjugated avidin (avidin-DTPA) were removed by centrifuge filtration through a device with a 10K cut-off limit. The avidin-DTPA was then reacted with Gd-(1-(2-naphthoyl)-3,3,3-trifluoroacetonate)_2_ to obtain avidin-GdDTPA (avidin-GdDTPA) as described above. Avidin-GdDTPA was separated from excess low molecular weight compounds as detailed above. On average, 12.5 GdDTPA groups were reported to be attached to each avidin molecule.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=avidin+Gd+in+vitro)]

For in vitro studies, NT-5 cells expressing HER-2/neu were derived from spontaneous mammary tumors of female HER-2/neu transgenic mice (13). In the same study, mouse carcinoma EMT-6 cells that do not express HER-2/neu were used as controls. Expression of HER-2/neu by the two cell lines was confirmed with fluorescence-activated cell-sorting analysis using appropriate reagents (13). The cells were exposed to biotinylated anti-HER-2/neu MAb in phosphate-buffered saline (PBS) containing bovine serum albumin (BSA) for 30 min at room temperature. The cells were then washed with PBS several times and incubated with avidin-GdDTPA for 5 min at room temperature. Control cells were exposed to a non-specific MAb or to avidin-GdDTPA. The cells were washed again as detailed above and fixed in 2% paraformaldehyde in PBS in a nuclear magnetic resonance tube. Subsequently, T1-weighted images (repetition time, TR = 1 s; spin echo time, TE = 8 ms) were obtained with an MRI probe. Only the NT-5 cells that were exposed to the biotinylated anti-HER-2/neu MAb showed a positive T1 contrast with avidin-GdDTPA, and the EMT-6 cells had a low background signal.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=avidin+Gd+rodentia)]

In vivo MRI studies were performed with severe combined immunodeficient mice bearing NT-5 and EMT-6 cell tumors (13). All experimental animals (n = 5/time point) were treated with the biotinylated anti-HER-2/neu antibodies, and the control animals bearing NT-5 tumors (n = 3) were treated with BSA in saline. The test animals were injected with the avidin-GdDTPA conjugate 12 h after the biotinylated MAb treatment. Control animals were given avidin-GdDTPA via intravenous injection. Parameters for the T1-weighted images were as follow: TR = 300 ms, TE = 15 ms, flip angle = 90° with a field view of 32 mm; 16 slice images were acquired over 15 min with a slice thickness of 2 mm. MRI images were obtained at 1, 8, 24, and 48 h after contrast treatment. The NT-5 tumors were reported to retain the contrast for 8–24 h after treatment, but the contrast decreased in the EMT-6 cell tumors 1 h after treatment. Also, the NT-5 tumors that were not pre-treated with the biotinylated MAb were reported to show no retention of the contrast agent. A statistically significant (P < 0.05) increase in signal was observed in the tumors treated with NT-5 (~1.7 relative units for the cells treated with NT-5 versus ~1 relative unit for the NT-5 control and EMT-6 cells) under these experimental conditions.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=avidin+Gd+non+primate+mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=avidin+Gd+non+human+primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=avidin+Gd+humans)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## NIH Support

Supported by NIH grant P20 CA86346

## References

1 Green N.M. (1990). Avidin and streptavidin. Methods Enzymol.
2 Holmberg A., Blomstergren A., Nord O., Lukacs M., Lundeberg J., Uhlen M. (2005). The biotin-streptavidin interaction can be reversibly broken using water at elevated temperatures. Electrophoresis.
3 Wilchek M., Bayer E.A., Livnah O. (2006). Essentials of biorecognition: the (strept)avidin-biotin system as a model for protein-protein and protein-ligand interaction. Immunol Lett.
4 Tong X., Smith L.M. (1992). Solid-phase method for the purification of DNA sequencing reactions. Anal Chem.
5 Hama Y., Urano Y., Koyama Y., Choyke P.L., Kobayashi H. (2007). Activatable fluorescent molecular imaging of peritoneal metastases following pretargeting with a biotinylated monoclonal antibody. Cancer Res.
6 Hama Y., Urano Y., Koyama Y., Kamiya M., Bernardo M., Paik R.S., Shin I.S., Paik C.H., Choyke P.L., Kobayashi H. (2007). A target cell-specific activatable fluorescence probe for in vivo molecular imaging of cancer based on a self-quenched avidin-rhodamine conjugate. Cancer Res.
7 Xu H., Regino C.A., Koyama Y., Hama Y., Gunn A.J., Bernardo M., Kobayashi H., Choyke P.L., Brechbiel M.W. (2007). Preparation and preliminary evaluation of a biotin-targeted, lectin-targeted dendrimer-based probe for dual-modality magnetic resonance and fluorescence imaging. Bioconjug Chem.
8 Kanehira K., Hu J., Pier T., Sebree L., Huang W. (2008). High endogenous avidin binding activity: an inexpensive and readily available marker for the differential diagnosis of kidney neoplasms. Int J Clin Exp Pathol.
9 Stipsanelli E., Valsamaki P. (2005). Monoclonal antibodies: old and new trends in breast cancer imaging and therapeutic approach. Hell J Nucl Med.
10 Barrett T., Koyama Y., Hama Y., Ravizzini G., Shin I.S., Jang B.S., Paik C.H., Urano Y., Choyke P.L., Kobayashi H. (2007). In vivo diagnosis of epidermal growth factor receptor expression using molecular imaging with a cocktail of optically labeled monoclonal antibodies. Clin Cancer Res.
11 Gee M.S., Upadhyay R., Bergquist H., Alencar H., Reynolds F., Maricevich M., Weissleder R., Josephson L., Mahmood U. (2008). Human breast cancer tumor models: molecular imaging of drug susceptibility and dosing during HER2/neu-targeted therapy. Radiology.
12 Sampath L., Kwon S., Ke S., Wang W., Schiff R., Mawad M.E., Sevick-Muraca E.M. (2007). Dual-labeled trastuzumab-based imaging agent for the detection of human epidermal growth factor receptor 2 overexpression in breast cancer. J Nucl Med.
13 Artemov D., Mori N., Okollie B., Bhujwalla Z.M. (2003). MR molecular imaging of the Her-2/neu receptor in breast cancer cells using targeted iron oxide nanoparticles. Magn Reson Med.
14 Lewis Phillips G.D., Li G., Dugger D.L., Crocker L.M., Parsons K.L., Mai E., Blattler W.A., Lambert J.M., Chari R.V., Lutz R.J., Wong W.L., Jacobson F.S., Koeppen H., Schwall R.H., Kenkare-Mitra S.R., Spencer S.D., Sliwkowski M.X. (2008). Targeting HER2-positive breast cancer with trastuzumab-DM1, an antibody-cytotoxic drug conjugate. Cancer Res.
15 Nahta R., Esteva F.J. (2007). Trastuzumab: triumphs and tribulations. Oncogene.
16 Artemov D., Mori N., Ravi R., Bhujwalla Z.M. (2003). Magnetic resonance molecular imaging of the HER-2/neu receptor. Cancer Res.
17 Reilly R.T., Gottlieb M.B., Ercolini A.M., Machiels J.P., Kane C.E., Okoye F.I., Muller W.J., Dixon K.H., Jaffee E.M. (2000). HER-2/neu is a tumor rejection target in tolerized HER-2/neu transgenic mice. Cancer Res.
18 Hnatowich D.J., Virzi F., Rusckowski M. (1987). Investigations of avidin and biotin for imaging applications. J Nucl Med.